# Daclizumab complexed to near-infrared fluorophore indocyanine green

Chemical name: | Daclizumab complexed to near-infrared fluorophore indocyanine green
Abbreviated name: | Dac-ICG
Synonym:
Agent Category: | Monoclonal antibody
Target: | Interleukin 2 receptor α chain (CD25)
Target Category: | Receptor
Method of detection: | Optical: Near-infrared (NIR) fluorescence
Source of signal / contrast: | Indocyanine green
Activation: | Yes
Studies: | - In vitro; - Rodents | Proposed structure of Daclizumab-indocyanine green conjugate.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=trastuzumab+indocyanine+green)]

The technique of non-invasive optical imaging is based on the principle that when a dye is exposed to light it absorbs energy and is elevated from the steady state to a high-energy state. To return to its normal, low-energy state, the molecule releases energy in the form of photons with wavelengths that are either in the visible (400–700 nm) or the near infrared (NIR; 700–900 nm) range (1). Although both types of dyes can be used for imaging, in general NIR agents are favored over those functional in the visible range because fluorescence from NIR probes can be detected in deep tissue, have low autofluorescence, and generate low background signals because tissues do not absorb in the NIR wavelength range (2). Among the various NIR agents, only one, indocyanine green (ICG; also known as IR-125 or Cardiogreen), with absorption at ~780 nm and emission at ~820 nm, is approved by the United States Food and Drug Administration (US FDA) for clinical applications (3) and is under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications. ICG is a tricarbocyanine dye that is fluorescent only in the free state and easily binds to proteins through non-covalent linkages (such as ionic, hydrophobic, electrostatic, or hydrogen bonds). When bound to proteins ICG is non-fluorescent, but on dissociation from the protein complex it reverts to the fluorescent state and the signal has been shown to be suitable for in vivo imaging (4).

The interleukin-2 (IL-2) receptor (IL2R) consists of three subunits (α, β, and γ) that are non-covalently linked. Among these subunits, the γ-chain is a constitutive component of the cell membrane, but the α- (also known as CD25) and β-chains have to be induced by IL-2 and other related ligands to bring about functionality to the receptor (5). The functions of the various subunits of IL2R and the signaling pathways used to mediate its activity are described elsewhere (5). Induction of the α-chain is believed to impart specificity to the receptor and indicates activation of the T cells and dendritic cells that participate in the development of an immune response and play a role in the progression of various malignancies and autoimmune diseases (6, 7). Once activated, the receptor-ligand complex is internalized by the cell for inactivation through enzymatic digestion in the lysosomes (8, 9). Because of its possible role in the development of allograft rejection, cancer, autoimmune diseases, etc., daclizumab (Dac), a commercially available humanized monoclonal antibody (MAb) directed toward the IL2R α-chain, is approved by the US FDA to prevent or treat renal allograft rejection (10). It is also under investigation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=daclizumab) for the treatment of a variety of ailments, including cancer.

The characteristic properties of ICG (fluorescent only in an unbound state) and the IL2R α-chain (internalization by the cell) prompted Ogawa et al. to develop an imaging probe for cancer by complexing ICG to Dac (Dac-ICG) (4). The investigators used the Dac-ICG complex to image cells that express the IL2R α-chain under in vitro conditions and showed that the complex could also be used for the imaging of IL2R α-chain–expressing xenograft tumors in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+synthesis)]

The synthesis of Dac-ICG was described by Ogawa et al. (4). ICG-N-hydroxysulfosuccinimide ester (ICG-sulfo-OSu) and Dac were obtained from commercial sources. Dac was incubated with ICG-sulfo-OSu (Dac:ICG ratio was either 1:1 or 1:5) in phosphate buffer (pH 8.5) for 30 min at room temperature. The Dac-ICG complex was purified on a PD-10 Sephadex G50 column with phosphate-buffered saline (PBS; pH not reported) as the elution buffer. With the reaction conditions used to generate the MAb-ICG complex, either oneor five ICG molecules (Dac-ICG(1:1) or Dac-ICG(1:5)) were reported to be bound to each Dac molecule, respectively.

For use as a control, a human polyclonal IgG-Cy5.5 complex was also synthesized in the manner described above. The storage conditions and stability of the various MAb-ICG complexes were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+in+vitro)]

Ogawa et al. performed fluorescence imaging with Dac-ICG(1:1) and Dac-ICG(1:5) solutions in PBS under in vitro conditions (4). Fluorescence of the two complexes was measured before and after exposure to a mixture of sodium dodecyl sulfate (SDS) and 2-mercaptoethanol (2-ME). Fluorescence was detected only in solutions exposed to the denaturing (SDS) and reducing (2-ME) agents. The Dac-ICG(1:5) solution exposed to SDS and 2-ME was reported to have a higher fluorescence compared to the Dac-ICG(1:1) solution under the same conditions, suggesting that the degree of fluorescence obtained from a dissociated MAb-ICG complex was proportionate to the number of ICG molecules bound to the MAb molecule. This indicated that dissociation of ICG from the MAb-ICG complex resulted in reversion of the dye from a non-fluorescent state to a fluorescent state.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+rodentia)]

Xenograft tumors were generated after subcutaneous (s.c.) injection of A431cells (of human skin carcinoma origin ) transfected either with the red fluorescent protein (A431/DsRed, used as control) or the IL2R α-chain (ATAC4 cells) in the right and left dorsum, respectively, of mice (n = 10 animals) for imaging studies (4). The Dac-ICG (1:1 or 1:5) complexes were respectively administered intravenously to the animals (n = 5 mice/Dac-ICG complex) through the tail vein 14–18 days after s.c. injection of the cells. Fluorescent imaging was performed on the mice 0–4 days after injection of the Dac-ICG complexes. During this period, fluorescence was observed only in the ATAC4 cell tumors, and the signal was higher with the Dac-ICG(1:5) complex versus the Dac-ICG(1:1) complex. Coinjection of the Dac-ICG(1:5) complex with the control IgG-Cy5.5 complex showed that all tumors were fluorescent with the non-specific Cy5.5 complex, but only the ATAC4 tumors were fluorescent with the Dac-ICG complex (fluorescence from the two dyes in the images was separated using appropriate software), indicating that the latter complex was specific for tumors expressing the IL2R α-chain. After treatment of the mice with the two Dac-ICG complexes, a steady increase in fluorescence with Dac-ICG(1:5) was reported in the ATAC4 tumors for 1 day (~150 autofluorescence units (au)), and it gradually decreased to ~100 au by day 4. During the same period, tumors of mice injected with the Dac-ICG(1:1) complex showed a steady fluorescence of ~20 au. A histological examination of the A431 and ATAC4 cell tumors using the hematoxylin and eosin stain showed that both tumor types had the same histology. No competition studies using animals pretreated with Dac were reported.

With observations from this study, the investigators concluded that the Dac-ICG complex could probably be adapted for tumor imaging in humans during surgery. However, they cautioned that the Dac-ICG complex could have a different toxicity compared with individual components of the complex, and extensive clinical testing of Dac-ICG would have to be performed before its application in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Trastuzumab+indocyanine+green+Human+Studies)]

No references are currently available.

## References

1 Sharma R., Wendt J.A., Rasmussen J.C., Adams K.E., Marshall M.V., Sevick-Muraca E.M. (2008). New horizons for imaging lymphatic function. Ann N Y Acad Sci.
2 Luker G.D., Luker K.E. (2008). Optical imaging: current applications and future directions. J Nucl Med.
3 Sakka S.G. (2007). Assessing liver function. Curr Opin Crit Care.
4 Ogawa, M., N. Kosaka, P.L. Choyke, and H. Kobayashi, In vivo Molecular Imaging of Cancer with a Quenching Near-Infrared Fluorescent Probe Using Conjugates of Monoclonal Antibodies and Indocyanine Green. Cancer Res, 2009
5 Gaffen S.L. (2001). Signaling domains of the interleukin 2 receptor. Cytokine.
6 Driesen J., Popov A., Schultze J.L. (2008). CD25 as an immune regulatory molecule expressed on myeloid dendritic cells. Immunobiology.
7 Ali E., Healy B., Stazzone L., Brown B., Weiner H., Khoury S. (2009). Daclizumab in treatment of multiple sclerosis patients. Mult Scler.
8 Woodman P. (2009). ESCRT proteins, endosome organization and mitogenic receptor down-regulation. Biochem Soc Trans.
9 Nabholz M., Combe M.C., Corthesy P., Lowenthal J., Gabathuler R. (1987). Interleukin 2 receptor traffic in a murine cytolytic T cell line. Eur J Immunol.
10 Kim S.E. (2009). Daclizumab treatment for multiple sclerosis. Pharmacotherapy.